# Pyro-Gly-Pro-Leu-Gly-Leu-Ala-Arg-Lys(BHQ3)

Chemical name: | Pyro-Gly-Pro-Leu-Gly-Leu-Ala-Arg-Lys(BHQ3)
Abbreviated name: | PP_MMP7_B
Synonym:
Agent category: | Peptide
Target: | Matrix metalloproteinase subtype-7 (MMP-7)
Target category: | Enzyme
Method of detection: | Optical imaging, near-infrared (NIR) fluorescence
Source of signal/contrast: | Pyropheophorbide α (Pyro)
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=PPMMP7B)]

Photodynamic therapy (PDT), also known as photochemotherapy, uses light-activated photosensitizers (PS) in the presence of oxygen to kill cells (1). PDT has become a promising modality to treat skin, esophagus, and lung cancers, as well as other diseases such as atherosclerosis, macular degeneration, and rheumatoid arthritis (2). In PDT, light excites the singlet state of the PS, followed by intersystem transition from the singlet state to the triplet state; then, the energy is transferred from the triplet state of the PS to the triplet ground state of oxygen, ^3^O_2_(X^3^Σ_g_^-^) (^3^O_2_ triplet state quenching) to generate singlet oxygen, ^1^O_2_(a^1^Δ_g_) (3). The produced ^1^O_2_ is a major cytotoxic agent that has a short life time (<200 ns) and an average diffusion range (~20 nm, which is smaller than the diameter of a cell) (2). Such a short diffusion range requires the delivery of target-specific PS agents into subcellular compartments such as cytoskeletal tubulin, lysosomes, mitochondria, plasma membrane, and the nucleus, where they can generate ^1^O_2_ efficiently (2). A novel type of PS agent, called a photodynamic molecular beacon (PMB) or killer beacon, has been developed to meet this requirement (2, 4). A typical PMB consists of four modular components: a fluorescent PS, a quencher, a linker, and a delivery vehicle. The target-specific linkers keep the fluorescent PS and the quencher within effective distance of the Föster radius (3–6 nm) (2), which allows efficient fluorescence resonance energy transfer between the fluorescent PS and the quencher. As a result, the fluorescent PS is silent until the PMB meets the target, where the enzyme cleaves the linker and activates the fluorescence of the PS (4). Thus, the PS performs two functions by producing ^1^O_2_ to kill cells and by illuminating detectable fluorescence to image its own therapeutic outcome (5).

Matrix metalloproteinases (MMPs) have been pharmaceutical targets for many years because they play important roles in many diseases such as atherosclerosis, lung pulmonary fibrosis, and cancer (4). MMPs in tumors aid the degradation of extracellular matrix, facilitate neoplastic cell motility, and direct cell invasion (4). Also known as matrilysin, MMP subtype-7 (MMP7) is one of only a few MMPs that are actually secreted by tumor cells (6). Pyro-Gly-Pro-Leu-Gly-Leu-Ala-Arg-Lys(BHQ3) (PP_MMP7_B) is a PMB specific for MMP7, and it is detectable with near-infrared (NIR) fluorescence imaging (4). PP_MMP7_B consists of the infrared fluorescence PS pyropheophorbide α (Pyro), a black hole quencher 3 (BHQ3), and a peptide linker (Gly-Pro-Leu-Gly-Leu-Ala-Arg-Lys (GPLGLARK)) (4). The peptide contains the tripeptide motif Pro-Leu-Gly for MMP7 recognition, and the cleavage site is located between the Gly and Leu residues. Pyro acts as the intracellular delivery vehicle and as the PS (absorption, 665 nm; emission, 675 nm and 720 nm) with good ^1^O_2_ production (50%). Pyro lacks dark toxicity (toxicity in absence of light) because of its low absorption between 450–600 nm. BHQ3 (absorption, 672 nm) can efficiently quench Pyro fluorescence via fluorescence resonance energy transfer (FRET). The cleavage of Pyro-Gly-Asp-Glu-Val-Asp-Gly-Ser-Gly-Lys(BHQ3) (PPB) by MMP7 separates the PS (Pyro) from the quencher (BHQ3) and restores the Pyro fluorescence for detection.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PPMMP7B)+AND+synthesis%0D%0A)]

Zheng et al. reported the detailed synthesis of PP_MMP7_B (4). A peptide of Fmoc-GPLGLAR(Pbf)K(Mtt)-Sieber resin (Pbf is 2,2,4,6,7-pentamethyldihydrobenzofuran-5-sulfonyl; Mtt is methyltrityl) was synthesized by the manual, Fmoc, solid-phase, peptide synthesis protocol with the use of commercially available N-α-protected amino acids as building blocks, Sieber amide resin as a solid support, and N-hydroxybenzotriazole (HOBt)/2-(benzotriazole-1-yl)-1,1,3,3-tetramethyluronium hexafluorophosphate (HBTU) as amino acid activators. After the last Fmoc group cleavage, Pyro-acid was coupled to the N-terminal glycine of the peptide-resin at a molar ratio of 3:1. The produced peptide resin was treated with 3% trifluoroacetic acid (TFA) and 5% triisopropylsilane (Tis) in dichloromethane to give Pyro-GPLGLAR(Pbf)K, followed by reaction with BHQ3-N-hydroxysuccinimide (NHS) to produce Pyro-GPLGLAR(Pbf)K(BHQ3). The resulting peptide was treated with 95% trifluoroacetic acid and 5% triisopropylsilane to produce PP_MMP7_B. The labeling was confirmed with ultraviolet-visible spectroscopy by identifying Pyro-specific absorbance at 414 nm and BHQ3-specific absorbance at 676 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PPMMP7B)+AND+%22in+vitro%22)]

The specificity of PP_MMP7_B to MMP-7 was tested in aqueous solution by measuring the fluorescence emitted from the Pyro in PP_MMP7_B and the production of singlet oxygen ^1^O_2_ induced by the activated Pyro (4). PP_MMP7_B emitted 15-fold less fluorescence than PP_MMP7_ (the positive control without attached BHQ3), which demonstrated an efficient quenching of Pyro fluorescence by BHQ3. In the presence of the enzyme MMP7, an immediate increase in the Pyro fluorescence of PP_MMP7_B was observed, which reached a plateau at 3 h with a 12-fold increase in fluorescence. However, in the presence of MMP2 or the co-presence of MMP7 and its inhibitor, no noticeable increase in Pyro fluorescence was observed. No cleavage by MMP7 occurred when PP_MMP7_B was replaced with its scrambled sequence (Pyro-GDEVDGSGK-BHQ3). The results were further confirmed with matrix-assisted laser desorption/ionization-time-of-flight mass spectrometry (MALDI-TOF). The production of ^1^O_2_ was evaluated through the NIR luminescence of ^1^O_2_ at 1,270 nm. ^1^O_2_ production in PP_MMP7_B was 18-fold lower than in PP_MMP7_ or in a mixture of PP_MMP7_ and BHQ3. This demonstrated that the close proximity of Pyro and BHQ3 to the self-folding of the MMP7-cleavable peptide effectively inhibited the ^1^O_2_ production of Pyro. Adding MMP7 to PP_MMP7_B restored the quenched ^1^O_2_ production by 19-fold, whereas the presence of MMP7 and its inhibitor prevented this restoration. This confirmed that MMP7 is suitable specifically for cleavage of PP_MMP7_B, which leads to the separation of Pyro and BHQ3 and the photo-activation of Pyro.

Zheng et al. used PP_MMP7_B to study MMP-7–triggered PDT in cancer cells in vitro (4). KB cells (human nasopharyngeal epidermoid carcinoma cells) with high MMP7 expression were used as MMP7^+^ cells, and BT20 cells (human breast cancer cell line) with deficient MMP7 expression were used as MMP7^-^ cells. After incubation with PP_MMP7_B or its scrambled sequence (Pyro-GDEVDGSGK-BHQ3 (C-PPB)), confocal microscopy was performed with excitation at 633 nm and detection at >650 nm. A strong fluorescence signal was observed in KB cells incubated with PP_MMP7_B, whereas minimal fluorescence was found in BT20 cells incubated with PP_MMP7_B and in KB cells or BT20 cells incubated with C-PPB. High-performance liquid chromatography was used to analyze the cell medium collected at the end of drug incubation, which demonstrated that the cleavage of MMP7 occurred in the KB cell medium and produced two fragments as found in the solution studies. No cleavages were found in the BT20 cell medium. These results suggest that the Pyro on PP_MMP7_B also serves as a delivery vehicle to cross the cell membrane in addition to being a fluorescence dye and a PS. The subcellular location of PP_MMP7_B and its cleaved fragments was examined with confocal microscopy via the measurement of Pyro fluorescence and MitoTracker (stain for mitochondria) fluorescence (4). The Pyro fragment of PP_MMP7_B was located in nearby mitochondria but was absent from the nucleus. The ^1^O_2_ production was evaluated through the measurement cell viability with the use of 3-(4,5-[underlined: di] (http://en.wikipedia.org/wiki/Di-) [underlined: methyl] (http://en.wikipedia.org/wiki/Methyl) [underlined: thiazol] (http://en.wikipedia.org/wiki/Thiazole)-2-yl)-2,5-di[underlined: phenyl] (http://en.wikipedia.org/wiki/Phenyl)tetrazolium bromide (MTT assay) in KB cells and BT20 cells before and after PDT treatment. Compared with cells not treated with drugs or light, no noticeable dark toxicity was found for treatment with up to 4 μM PP_MMP7_B or C-PPB. Upon PDT treatment, only PP_MMP7_B reduced the viability of the KB cells. To further confirm whether this PDT-induced cytotoxicity occurred via the apoptotic mechanism, Apoptag Plus in situ fluorescein was used to stain the KB cells. KB cells with PP_MMP7_B and PDT treatment demonstrated a strong signal in the Apoptag fluorescein channel (excitation, 488 nm; emission, 497–580 nm), whereas KB cells with PP_MMP7_B but without PDT treatment exhibited no significant apoptosis, which suggests that apoptosis may be the primary cytotoxic mechanism.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PPMMP7B) +AND++rodentia)]

Zheng et al. studied the cleavage of PP_MMP7_B in vivo with fluorescence imaging (4). A mouse bearing two KB tumors (one on each flank) was injected intravenously with 80 nmol PP_MMP7_B. Compared with the prescan images or with the drug-free mouse, no increase in Pyro fluorescence was observed immediately after injection. However, the fluorescence in the tumor increased 20 min later and peaked at 3 h, indicating MMP7-triggered PP_MMP7_B activation. At 3 h, PDT treatment was administered to the tumor on the left flank, whereas the tumor on the right flank served as a dark control. One hour after PDT treatment (4 h after injection), the treated tumor became edematous, whereas the untreated tumor showed no changes in size or fluorescence. For comparison, a drug-free mouse bearing two tumors was treated in the same way; no changes in size or fluorescence were observed in either tumor. Three days after PDT, the treated tumor in the drugged mouse decreased in size, whereas the untreated tumor and both tumors in the drug-free mouse continued to grow. These data demonstrate that PP_MMP7_B that accumulated in MMP7^+^ tumors is photodynamically activatable.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PPMMP7B) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=( PPMMP7B) +AND+human)]

No publication is currently available.

### NIH Support

CA 95330

## References

1 Dougherty T.J., Gomer C.J., Henderson B.W., Jori G., Kessel D., Korbelik M., Moan J., Peng Q. (1998). Photodynamic therapy. J Natl Cancer Inst.
2 Stefflova K., Chen J., Zheng G. (2007). Killer beacons for combined cancer imaging and therapy. Curr Med Chem.
3 Clo E., Snyder J.W., Voigt N.V., Ogilby P.R., Gothelf K.V. (2006). DNA-programmed control of photosensitized singlet oxygen production. J Am Chem Soc.
4 Zheng G., Chen J., Stefflova K., Jarvi M., Li H., Wilson B.C. (2007). Photodynamic molecular beacon as an activatable photosensitizer based on protease-controlled singlet oxygen quenching and activation. Proc Natl Acad Sci U S A.
5 Stefflova K., Chen J., Marotta D., Li H., Zheng G. (2006). Photodynamic therapy agent with a built-in apoptosis sensor for evaluating its own therapeutic outcome in situ. J Med Chem.
6 Overall C.M., Kleifeld O. (2006). Tumour microenvironment - opinion: validating matrix metalloproteinases as drug targets and anti-targets for cancer therapy. Nat Rev Cancer.